# Cy5.5-Poly-L-lysine-methoxypolyethylene glycol

Chemical name: | Cy5.5-Poly-L-lysine-methoxypolyethylene glycol
Abbreviated name: | Cy5.5-PL-MPEG, Cy5.5-PGC
Synonym:
Agent Category: | Copolymers
Target: | Cathepsin B
Target Category: | Enzyme binding
Method of detection: | Optical, near-infrared fluorescence
Source of signal/contrast: | Cy5.5
Activation: | Yes
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=63102437), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=66346650) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=1508) for more information about cathepsin B.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG)]

Optical fluorescence imaging is increasingly used to study biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (650–900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (3). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (4). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (5).

Several families of proteases are involved in atherogenesis, myocardial infraction, angiogenesis, and tumor invasion and metastases (6-9). The cysteine proteases (cathepsin B, H, and L) and serine protease (cathepsin D) are present in the intracellular endosomal system of cells such as macrophages, epithelial cells, and tumor cells. These proteases participate in degradation of ECM and remodeling of tissues. A synthetic protected graft copolymer (PGC) consisting of poly-L-lysine (PL) with multiple methoxypolyethylene glycol (MPEG) side chains has been used as a drug carrier with efficient accumulation in tumor (10, 11). Weissleder et al. (12) attached multiple Cy5.5 NIR dye molecules to the unmodified PL side chains to form a fluorescence-quenched polymer, Cy5.5-PL-MPEG (Cy5.5-PGC). The Cy5.5 molecules are in close proximity, which results in fluorescence quenching because of efficient fluorescence resonance energy transfer. The NIR fluorescence signal will increase when the lysine-lysine bond is cleaved by proteases, releasing fragments that contain Cy5.5. Cy5.5 is a NIR fluorescent dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^. Cy5.5-PGC is being developed for NIR fluorescence imaging of cathepsin B proteolytic activity in tumors, atherosclerosis, and other diseases.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+synthesis)]

PL-MPEG was formed by a reaction of the hydroxysuccinimide ester of methoxypolyethylene glycol succinate to the ω-NH_2_ group of PL (35.5 kDa) (12). The purified PL-MPEG had a calculated average molecular mass of 480 kDa as determined with elemental analysis. The PL-MPEG was then further modified with Cy5.5-hydroxysuccinimide ester via the unmodified ω-NH_2_ group of PL. Cy5.5-PGC was purified with column chromatography. Each PL backbone contained an average of 92 MPEG molecules and 11 molecules of Cy5.5 and yielded (Cy5.5)_11_-PL-MPEG_92_ (Cy5.5-PGC), which contained 44 unmodified L-lysine moieties on the backbone as sites for cleavage by enzymes with lysine-lysine specificity.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+and+in+vitro)]

Weissleder et al. (12) showed that Cy5.5-PGC was activated by trypsin and subcellular fractions (Golgi and high-density lysosomes) from human LX-1 small-cell carcinoma cell homogenates. NIR fluorescence of Cy5.5-PGC was 15-fold lower than free Cy5.5 at equimolar concentration. Cysteine protease, trypsin, and trypsin-like serine protease inhibitors inhibited the activation of the probe by the protease-rich subcellular fractions. On the other hand, a cathepsin D inhibitor showed no inhibition. Furthermore, fluorescence microscopy showed that the probe was internalized (ng PGC/μg cellular protein) by C6 glioma (1.31 ± 0.11), 9L gliosarcinoma (1.90 ± 0.20), R13762 adenocarcinoma (6.72 ± 0.37), LX-1 (6.78 ± 0.38), MCF-7 mammary adenocarcinoma (6.08 ± 0.09), and LS174T colon adenocarcinoma (1.81 ± 0.10) after 15 min of incubation. Chen et al. (13) showed that there was a 50-fold increase in NIR signal after incubation with purified cathepsin B but little activation by other cathepsins (H, D, and L). The probe was not activated by serum or whole blood up to 24 h of incubation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+rodentia)]

Weissleder et al. (12) performed biodistribution studies of Cy5.5-PGC in nude mice bearing a LX-1 subcutaneous xenograft. Images were obtained up to 96 h after i.v. injection of 10 μmol Cy5.5/mouse of Cy5.5-PGC. Substantial contrasts were observed between LX-1 tumors (<0.3–2 mm) and normal tissue. Ex vivo imaging showed that most of the NIR fluorescence signal intensity was from the LX-1 tumor (812 ± 125 AU), spleen (626 ± 72 AU), and liver (2,163 ± 226 AU). No blocking or cathepsin B inhibition experiment was performed.

Chen et al. (13) performed in vivo imaging of atherosclerosis in apolipoprotein E–deficient (apoE^-/-^) mice using Cy5.5-PGC fluorescence-mediated tomography. Marked fluorescence signal could be detected in the aortic arch and abdominal aorta of the apoE^-/-^ mice at 24 h after i.v. injection of 5 nmol of Cy5.5-PGC. Ex vivo imaging showed that the NIR fluorescence signal intensity was higher in the arch and abdominal aortic lesions of apoE^-/-^ mice compared with the unaffected aorta of control wild-type mice (P < 0.001). Cathepsin B immunohistochemistry and reverse transcription confirmed that the overexpression of cathepsin B colocalized with NIR signal in the lesions. Furthermore, immunofluorescence also colocalized with immunoreactivity for Mac-3, a macrophage marker. No blocking or cathepsin B inhibition experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+human)]

No publication is currently available.

## NIH Support

R01 CA74424-01

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
4 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
5 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
6 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
7 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
8 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
9 Brix K., Dunkhorst A., Mayer K., Jordans S. (2007). and Cysteine cathepsins: Cellular roadmap to different functions. Biochimie.
10 Marecos E., Weissleder R., Bogdanov A. (1998). Antibody-mediated versus nontargeted delivery in a human small cell lung carcinoma model. Bioconjug Chem.
11 Weissleder R., Cheng H.C., Marecos E., Kwong K., Bogdanov A. (1998). Non-invasive in vivo mapping of tumour vascular and interstitial volume fractions. Eur J Cancer.
12 Weissleder R., Tung C.H., Mahmood U., Bogdanov A. (1999). In vivo imaging of tumors with protease-activated near-infrared fluorescent probes. Nat Biotechnol.
13 Chen J., Tung C.H., Mahmood U., Ntziachristos V., Gyurko R., Fishman M.C., Huang P.L., Weissleder R. (2002). In vivo imaging of proteolytic activity in atherosclerosis. Circulation.